# ^99m^Tc-Labeled, PEGylated (N^α^His)Ac-β^3^hLys-βAla-βAla-Gln^7^-Trp^8^-Ala^9^-Val^10^-Gly^11^-His^12^-Cha^13^-Nle^14^-NH_2_

Chemical name: | ^99m^Tc-Labeled, PEGylated (N^α^His)Ac-β^3^hLys-βAla-βAla-Gln^7^-Trp^8^-Ala^9^-Val^10^-Gly^11^-His^12^-Cha^13^-Nle^14^-NH_2_
Abbreviated name: | ^99m^Tc-PEG_x_-Lys-BN (x = 5, 10, and 20 kDa)
Synonym: | ^99m^Tc-PEG_5_-Lys-BN, ^99m^Tc-PEG_10_-Lys-BN, and ^99m^Tc-PEG_20_-Lys-BN
Agent Category: | Peptides
Target: | Gastrin-releasing peptide receptors (GRPR)
Target Category: | Receptors
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure available

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bombesin%20and%20molecular%20imaging)]

The ^99m^Tc-labeled, PEGylated (N^α^His)Ac-β^3^hLys-βAla-βAla-Gln^7^-Trp^8^-Ala^9^-Val^10^-Gly^11^-His^12^-Cha^13^-Nle^14^-NH_2_ (Lys-BN), abbreviated as ^99m^Tc-PEG_x_-Lys-BN (x = 5, 10, and 20 kDa), are PEGylated bombesin (BN) analogs that were synthesized by Dapp et al. for imaging of tumors that overexpress gastrin-releasing peptide receptors (GRPR) (1).

Engineered proteins and peptides are widely applied in the development of molecular imaging agents; however, they exhibit some unfavorable pharmacokinetic properties when used in vivo, such as rapid clearance, immunogenicity, and poor stability (e.g., aggregation, degradation, deamination, oxidation, etc.) (2, 3). As a technique to overcome these limits of proteins and peptides, PEGylation has been extensively studied recently, and the number of agents newly developed with PEGylation is increasing continuously (3, 4). PEGylation is defined as the covalent attachment of poly(ethylene glycol) (PEG) chains to bioactive substances (3). PEG possesses three key properties: great flexibility due to the absence of bulky substituents along the chain; high hydration of the polymeric backbone; and a high degree of safety, with toxicity only at very high doses (1, 3, 4). Furthermore, PEG can be coupled with virtually any exposed surface and even some buried amino acids in a protein, and this coupling can be achieved at the N- or C-terminus, the cysteines located far from the receptor-binding site, or the incorporated unnatural amino acids. PEG increases the blood circulation of a given protein by increasing its hydrodynamic volume, prevents its immunogenicity, reduces its aggregation, and increases its thermal stability. However, a reduction in biological potency is common after PEGylation because of the steric entanglement of polymer chains during the protein/receptor recognition process (3). This reduction is also related to the PEGylation methods and PEG selected. The properties of PEG vary significantly with molecular weight and concentration.

Radiolabeled BN analogs are promising radiotracers for tumor imaging and therapy by targeting GRPR (5-7). However, the low in vivo stability of BN analogs limits their clinical application (8, 9). Dapp et al. prepared a series of PEGylated BN(7-14) analogs and evaluated their properties in vitro and in vivo (1). PEGylation was performed with linear PEG molecules of various sizes (5 kDa (PEG_5_), 10 kDa (PEG_10_), and 20 kDa (PEG_20_)) through the ɛ-amino group of a β^3^hLys-βAla-βAla spacer between the BN sequence and the (N^α^His)Ac chelator. In vitro results showed that PEGylation did not affect the binding affinity of BN analogs, but it did slow their binding kinetics (1). In vivo results showed that PEGylation increased the stability of the analogs, improved their pharmacokinetics, and enhanced the tumor retention.

### Related Resource Links:

Bombesin-based imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=bombesin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Bombesin-based clinical trials (http://clinicaltrials.gov/ct2/results?term=bombesin)

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=GRPR) and protein (http://www.ncbi.nlm.nih.gov/protein?term=GRPR) sequences of GRPR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21982571)]

The BN peptide Lys-BN was synthesized with peptide solid-phase synthesis (1). Methoxypolyethylene glycol succinimidyl esters (MeO-PEG-NHS; 5, 10, and 20 kDa) were commercially available. To PEGylate the BN peptides, MeO-PEG-NHS was mixed with each BN analog and incubated for 1 h at room temperature. More MeO-PEG-NHS was added after 30 min and again after 45 min. The solvents were removed by evaporation, and the final product was dissolved in water before labeling with ^99m^Tc. The yields of PEG_x_-Lys-BN analogs were 85%, 74%, and 46% for PEG_5_, PEG_10_, and PEG_20_, respectively. The molecular weight was 1,441.9 for Lys-BN, 6,335.1 for PEG_5_-Lys-BN, 10,945.4 for PEG_10_-Lys-BN, and 22,709.5 for PEG_20_-Lys-BN.

To label ^99m^Tc, a solution of Na[^99m^TcO_4_], sodium boranocarbonate, borax, potassium sodium tartrate tetrahydrate, and sodium carbonate was heated for 40 s at 150°C. After adjusting the pH to 6.5, the solution was mixed with the PEGylation analogs and heated for 2 min at 90°C. The non-PEGylated Lys-BN was similarly labeled with ^99m^Tc. High-performance liquid chromatography was performed to separate the non-PEGylated from the PEGylated ^99m^Tc-labeled peptides, and the ^99m^Tc-labeled from the unlabeled peptides on the basis of the difference of their retention times. The radiochemical purities and specific radioactivities for both ^99m^Tc-Lys-BN and ^99m^Tc-PEG-Lys-BN analogs were >95% and 5.02 TBq/μmol (135.7 Ci/μmol), respectively (1). The radiochemical yields for the analogs were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21982571)]

The octanol/phosphate-buffered saline partition coefficients (log D) were determined at pH 7.4, and the log D values were −0.74 ± 0.06, −1.61 ± 0.30, −1.05 ± 0.16, and −1.08 ± 0.25 for ^99m^Tc-Lys-BN, ^99m^Tc-PEG_5_-Lys-BN, ^99m^Tc-PEG_10_-Lys-BN, and ^99m^Tc-PEG_20_-Lys-BN, respectively, showing that PEGylation resulted in increased hydrophilicity of the analogs (1).

The in vitro stability was evaluated after 24 h of incubation with human plasma (1). The analog ^99m^Tc-Lys-BN was rapidly degraded, with only 16.6 ± 2.3% intact at 24 h. In contrast, all PEGylated BN analogs remained intact. The half-life of ^99m^Tc-Lys-BN was 11.4 h, whereas the half-lives of the PEGylated BN analogs were >24 h. The cell binding assay confirmed these results (1). With the analogs obtained after incubation with human plasma for 24 h, the specific binding of the ^99m^Tc-Lys-BN to PC-3 cells was reduced to 17.2 ± 1.9% in comparison to the specific binding without incubation in human plasma. The percentages of the PEGylated BN analogs after 24 h of incubation with human plasma were still 115.5 ± 18.3%, 96.0 ± 3.2%, and 99.9 ± 4.9% for ^99m^Tc-PEG_5_-Lys-BN, ^99m^Tc-PEG_10_-Lys-BN, and ^99m^Tc-PEG_20_-Lys-BN, respectively.

Saturation binding assays were performed with PC-3 cells to evaluate the binding kinetics of the ^99m^Tc-labeled analogs (1). The dissociation constants (K_d_) for ^99m^Tc-PEG-Lys-BN analogs were 0.89 ± 0.32, 0.53 ± 0.04, and 0.63 ± 0.20 nM for PEG_5_, PEG_10_, and PEG_20_, respectively. These values were in the same range as the K_d_ value of Lys-BN, which was 0.65 ± 0.35 nM. Compared to the non-PEGylated ^99m^Tc-Lys-BN, the PEGylated forms had slower binding kinetics.

On cell internalization, all analogs showed specific, time-dependent cell uptake (1). ^99m^Tc-Lys-BN internalized rapidly, reached its maximum within the first 30 min of incubation (~30% per 10^6^ cells), and remained virtually constant for about 2 h. All PEGylated analogs showed lower internalization into PC-3 cells, and longer incubation was required to reach the plateau (between 4 h and 24 h). The size of the PEG entity had an influence on the amount of internalized fraction. After incubation for 4 h, the internalization rates were 2.9 ± 0.9%, 1.7 ± 1.4%, and 1.2 ± 1.2% for ^99m^Tc-PEG_5_-Lys-BN, ^99m^Tc-PEG_10_-Lys-BN, and ^99m^Tc-PEG_20_-Lys-BN, respectively.

On cell externalization, ^99m^Tc-Lys-BN was externalized quickly, with 73.37 ± 1.30% of the internalized activity released within the first 2.5 h, and only 21.44 ± 2.09% of the internalized fraction remained in the cells after 24 h. In contrast, the externalization of PEGylated analogs was slower, with 80.2 ± 3.7% (^99m^Tc-PEG_5_-Lys-BN), 42.8 ± 0.9% (^99m^Tc-PEG_10_-Lys-BN), and 54.2 ± 12.1% (^99m^Tc-PEG_20_-Lys-BN) of the internalized fraction remaining in the cells after 24 h (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21982571)]

The effect of PEGylation on in vivo stability was tested in Balb/c mice after injection of the radiolabeled BN analogs (10–20 MBq (0.27–0.54 mCi)) (n = 2 mice/time point) (1). The non-PEGylated ^99m^Tc-Lys-BN was rapidly metabolized in mice, with only 5.28 ± 0.06% intact at 5 min and no intact ^99m^Tc-Lys-BN at 30 min after injection in blood. ^99m^Tc-PEG_5_-Lys-BN showed higher stability in vivo than ^99m^Tc-Lys-BN, with 13.20 ± 1.59% intact at 5 min and 4.38 ± 0.60% intact at 30 min after injection. No data were reported for ^99m^Tc-PEG_10_-Lys-BN and ^99m^Tc-PEG_20_-Lys-BN.

The effect of PEGylation on biodistribution was tested in mice bearing PC-3 tumor xenografts after injection of 0.5–3.5 MBq (13.51–94.59 µCi) of the analogs (Table 1) (1). Mice (n = 3–6/group) were euthanized at 1, 4, and 24 h after injection. The radioactivity in each tissue was determined and expressed as a percentage of injected dose per gram of tissue (% ID/g).

The blood clearance of ^99m^Tc-Lys-BN was fast. Conjugation with PEG_5_ did not affect the blood clearance of the BN analog, whereas conjugation with PEG_10_ and especially PEG_20_ led to longer blood circulation times and slower clearance rates (P < 0.01) (1).

The highest tumor uptake values for ^99m^Tc-Lys-BN, ^99m^Tc-PEG_10_-Lys-BN, and ^99m^Tc-PEG_5_-Lys-BN were found 1 h after injection (2.80%, 1.79%, and 3.91% ID/g, respectively), with the uptake of ^99m^Tc-PEG_5_-Lys-BN being significantly higher than that of ^99m^Tc-Lys-BN (P < 0.05). The highest tumor uptake for ^99m^Tc-PEG_20_-Lys-BN, however, was found 4 h after injection (4.86% ID/g). The tumor washout was slower for the PEGylated analogs; only 0.53% ID/g of the ^99m^Tc-Lys-BN remained in the tumor, whereas 1.73%, 1.14%, and 4.12% ID/g were found at 24 h after injection for the PEG_5_, PEG_10_ and PEG_20_ analogs, respectively.

^99m^Tc-PEG_5_-Lys-BN showed the highest tumor/nontarget ratios at all time points, especially at 24 h after injection. Compared to the non-PEGylated ^99m^Tc-Lys-BN, PEG_10_ did not lead to improved tumor/nontarget ratios, while PEG_20_ improved tumor/kidney ratios (2- and 4-fold increase at 4 h and 24 h after injection, respectively) and tumor/liver ratios (2- and 3-fold increase at the same time points, respectively).

In the GRPR-expressing pancreas, all analogs showed highest uptake at 1 h after injection, but there was no statistical difference in uptake between PEGylated and non-PEGylated analogs. In the GRPR-expressing colon, the uptake was different for the PEGylated and non-PEGylated analogs. ^99m^Tc-PEG_5_-Lys-BN and ^99m^Tc-PEG_10_-Lys-BN showed significantly lower colon uptake, while ^99m^Tc-PEG_20_-Lys-BN and ^99m^Tc-Lys-BN showed comparable uptake.

In the liver, the highest uptake was observed with ^99m^Tc-Lys-BN at 1 h after injection (3.92% ID/g); however, its clearance was relatively fast, with only 0.56% ID/g of the radioactivity remaining at 24 h after injection. ^99m^Tc-PEG_5_-Lys-BN exhibited a significantly lower liver uptake at all time points (<1% ID/g). ^99m^Tc-PEG_10_-Lys-BN showed lower liver uptake at early time points but slow clearance. There was no difference in the liver uptake between ^99m^Tc-PEG_20_-Lys-BN and ^99m^Tc-Lys-BN.

Accumulation in the kidney and washout from the kidneys were similar for both ^99m^Tc-Lys-BN and ^99m^Tc-PEG_5_-Lys-BN. Despite a slightly lower accumulation of ^99m^Tc-PEG_10_-Lys-BN in the kidneys (4.10% ID/g at 1 h after injection), the accumulated radioactivity was cleared slowly, with 2.16% ID/g found at 24 h after injection. ^99m^Tc-PEG_20_-Lys-BN showed the highest kidney uptake at all time points and the slowest clearance from kidney.

Table 1: Influence of PEGylation on the biodistribution of BN analogs

Organ | ^99m^Tc-Lys-BN | ^99m^Tc-PEG_5_-Lys-BN | ^99m^Tc-PEG10-Lys-BN | ^99m^Tc-PEG_20_-Lys-BN
Blood | 0.96 ± 0.30 | 1.00 ± 0.08 | 3.70 ± 0.26 | 14.46 ± 1.27
Kidneys | 5.79 ± 0.95 | 5.09 ± 1.83 | 4.10 ± 0.26 | 7.73 ± 0.48
Pancreas | 13.75 ± 2.32 | 12.92 ± 0.53 | 9.43 ± 1.94 | 12.42 ± 1.23
Colon | 4.94 ± 0.65 | 2.04 ± 0.68 | 2.27 ± 0.27 | 4.35 ± 0.86
Liver | 3.92 ± 0.39 | 0.64 ± 0.06 | 2.03 ± 0.22 | 3.61 ± 0.36
Tumor | 2.80 ±0.28 | 3.91 ± 0.44 | 1.79 ± 0.39 | 2.79 ± 0.34

*Data were obtained at 1 h after injection of analogs (n = 3-4)

Blocking studies were performed at 1 h after co-injection of unlabeled BN(1-14) (100 μg) and radiolabeled analogs (n = 3 mice) (1). The uptake in the GRPR-expressing tissues, such as the pancreas, colon, and tumor, was markedly reduced. The uptake of the non-PEGylated BN analog was inhibited the most, while the inhibition was less effective for the PEGylated analogs in a size-dependent manner. The pancreas and colon uptake values were reduced by 54%–95% and 50%–86%, respectively, and no inhibition was found for ^99m^Tc-PEG_20_-Lys-BN. The tumor uptake was significantly inhibited for ^99m^Tc-Lys-BN and ^99m^Tc-PEG_5_-Lys-BN (70% and 58% reduction, respectively). However, no significant differences were found in the tumor uptake of ^99m^Tc-PEG_10_-Lys-BN and ^99m^Tc-PEG_20_-Lys-BN for the blocked and the unblocked groups.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Dapp S., et al. (2011). PEGylation of (99m)Tc-labeled bombesin analogues improves their pharmacokinetic properties. Nucl Med Biol.
2 Gronwall C., Stahl S. (2009). Engineered affinity proteins--generation and applications. J Biotechnol.
3 Pasut, G. and F.M. Veronese, State of the art in PEGylation: The great versatility achieved after forty years of research. J Control Release, 2011
4 Jokerst J.V., et al. (2011). Nanoparticle PEGylation for imaging and therapy. Nanomedicine (Lond).
5 Ananias H.J., et al. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
6 Cescato R., et al. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
7 Ischia J., et al. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
8 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
9 Schroeder R.P., et al. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.